# Mono-[^123^I]iodohypericine monocarboxylic acid

Chemical name: | Mono-[^123^I]iodohypericine monocarboxylic acid
Abbreviated name: | [^123^I]MIHA
Synonym: | [^123^I]16-iodo-3-methyl-hexadecanoic acid
Agent Category: | Compound
Target: | Necrotic tissue
Target Category: | Uptake
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of Signal/Contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem.

## Background

[PubMed]

The myocardial perfusion imaging technique is often used to diagnose acute myocardial infarction (AMI) with either positron emission tomography (PET) or single-photon emission computed tomography (SPECT) with the use of radiopharmaceuticals, but all these agents have limitations as described in detail by Cuocolo et al. (1). It is well known that a rapid diagnosis of AMI is important to develop a suitable treatment and increase the chances of a favorable outcome. The use of scintigraphic agents such as pyrophosphate labeled with radioactive technetium (^99m^Tc), which targets the calcium phosphate deposit in the myocardial tissue or the F(ab) fragment of an anti-myosin antibody (labeled with radioactive indium), and ^99m^Tc-labeled glucarate has been attempted in the diagnosis of AMI, but the diagnostic performance of these agents is not entirely satisfactory (2). The pyrophosphate shows a low affinity and specificity for the necrotic myocardium in AMI patients, and the anti-myosin antibody is no longer available commercially (2). Although [^99m^Tc]glucarate appears to be a promising agent for the detection and quantification of AMI, this agent is rapidly washed out from the infarcted myocardium, which means that a meaningful scan can be obtained only for a short time (<9 h) after the infarct has occurred because [^99m^Tc]glucarate targets positively charged histones that disintegrate rapidly in the necrotic tissue (2). Another promising radiochemical used for the detection and diagnosis of AMI is [^123^I]-β-methyl iodophenyl-pentadecanoic acid (alos known as mono iodohypericin carboxylic acid or MIHA), a fatty acid derivative labeled with radioactive iodine (^123^I); this agent has been widely used in Japan and Europe for SPECT imaging of the heart and is undergoing clinical evaluation in the United States (3-5).

It has been shown that photosensitizer porphyrin derivatives specifically target the necrotic tissue found in neoplastic tumors and can be used in photodynamic therapy of cancer (6). Because porphyrins bind primarily to necrotic tissue, these compounds could be used as magnetic resonance imaging contrast agents to visualize AMI under preclinical conditions (7, 8). Bearing this in mind, investigators have evaluated the use of hypericin, a polycyclic polyaromatic quinone found in the St. John's wort plant (Hypericum perforatum) that has a chemical structure similar to some porphyrin derivatives, for the detection and imaging of necrotic tissue, including AMI-caused necrotic tissue (9-12). To achieve this, hypericin was derivatized with radioactive iodine (^123^I) to mono-[^123^I]iodohypericin ([^123^I]MIH) and used in the imaging studies with SPECT (9-12). In these studies, the investigators observed that [^123^I]MIH had a slow plasma clearance under in vivo conditions, probably because it has a lipophilic character, and AMI was not visualized for at least 2 h after treatment with the radiochemical (13). The investigators hypothesized that a hypericine derivative with low lipophilicity would be cleared faster from circulation and allow early visualization of necrotic tissue. The investigators derivatized [^123^I]MIH to a monocarboxylic acid ([^123^I]MIHA), which has a lower lipophilicity than MIH, and evaluated this new agent for the detection of necrotic tissue in rats with ethanol-induced liver necrosis (13).

## Synthesis

[PubMed]

The synthesis of [^123^I]MIHA was described in detail by Fonge et al. (13). Briefly, emodin, a precursor of hypericin, was acetylated to produce triacetyl-emodin, which was oxidized to obtain triacetyl-emodic acid. The triacetyl-emodic acid was mixed with emodin in presence of hydroquinone (serving as a free radical scavenger) to yield protohypericin monocarboxylic acid. The protohypericin derivative was photocyclized by irradiation with a 400-W halogen lamp for 30 min to obtain hypericin monocarboxylic acid, which was used as a precursor to synthesize MIHA by an electrophilic substitution reaction using sodium iodide (NaI) with peracetic acid as the oxidizing agent.

To produce [^123^I]MIHA, protohypericin monocarboxylic acid was radioiodinated by the successive addition of ethanol, phosphoric acid, peracetic acid, and Na[^123^I]. The mixture was incubated at room temperature for 30 min and photocyclized for 30 min with a 400-W halogen lamp. [^123^I]MIHA was purified with reverse-phase high-performance liquid chromatography coupled with a radiometric detector on an XTerra C_18_ column. The radiochemical yield was >75% relative to the initial ^123^I activity. The specific activity of the radiochemical was 950 GBq/μmol (25.67 Ci/μmol). The radiochemical purity and stability of [^123^I]MIHA was not provided (13).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed]

An isolated, isovolumically beating rabbit heart under ischemic conditions was used to study the myocardial kinetics of [^123^I]MIHA (14). The investigators reported that the early retention fraction of MIHA under these conditions was dependent on the coronary flow, and the early retention fraction was higher under ischemic conditions than that of the normal controls (0.24 ± 0.10 and 0.14 ± 0.04, respectively, P = 0.004).

## Animal Studies

### Rodents

[PubMed]

Normal NMRI mice were used in a preliminary investigation of [^123^I]MIHA biodistribution after a tail vein injection of the radiochemical (13). For comparison, [^123^I]MIH was injected into another group of mice through the same route. The animals from both groups were euthanized at various time points between 30 min and 24 h after injection (n = 4 mice per time point). Organs were removed from the animals and weighed, and the incorporated radioactivity was counted. Although both radiochemicals had a high incorporation in the liver, the uptake of [^123^I]MIH in this organ was higher than that of [^123^I]MIHA at all time points, indicating that the tracers were cleared primarily through the hepatobiliary route. The blood clearance of [^123^I]MIHA at 4 h (0.6% of injected dose/gram tissue (% ID/g)) was higher than that of [^123^I]MIH at 4 h (28.2% ID/g). Compared to [^123^I]MIH (<6% ID/g) the clearance of [^123^I]MIHA (21.1% ID/g) was primarily through the kidneys at 24 h (13).

The affinity of [^123^I]MIHA was studied in seven Wistar rats with hepatic necrosis induced by slow infusion of ethanol into the left lobe of the liver (13). The viable right lobe served as the control. The rats were injected with [^123^I]MIHA and euthanized at 4 h (n = 4 animals) and 24 h (n = 3 animals) after injection. Both liver lobes were harvested from all animals and washed with saline, and absorbed radioactivity was counted. The tissues were subsequently frozen, and serial microtome sections were mounted on slides for autoradiography and confirmation with hematoxylin and eosin (H & E) staining. The incorporated radioactivity ratio of necrotic tissue versus viable tissue in terms of [^123^I]MIHA uptake was 1.2 and 1.9 at 4 and 24 h, respectively. There was a good match between the uptake of [^123^I]MIHA, as viewed by autoradiography, and the H & E staining of the necrotic liver sections (13). From these observations the investigators concluded that [^123^I]MIHA was suitable for use in the detection of tissue necrosis.

### Other Non-Primate Mammals

[PubMed]

No references are currently available.

### Non-Human Primates

[PubMed]

No references are currently available.

## Human Studies

[PubMed]

Marie et al. investigated the exercise SPECT defect (SPECT with thallium (^201^Tl)) observed in patients with either necrotic (n = 13 individuals) or chronically ischemic and viable (n = 15 individuals) myocardium after two consecutive injections of [^123^I]MIHA (14). Imaging was performed 15–35 min after the first injection of [^123^I]MIHA, and the uptake was significantly higher in the ischemic areas (74 ± 9% of the maximal left ventricle value) than in the necrotic areas (59 ± 7%; P = 0.0001) and lower than in the normal areas (88 ± 6%; P = 0.0001). Similar results were obtained after the second round of SPECT imaging (14). However, the investigators observed no change in the [^123^I]MIHA clearance in consecutive SPECT studies with these patients.

## Supplemental Information

[Disclaimers]

## References

1 Cuocolo A., Acampa W., Imbriaco M., De Luca N., Iovino G.L., Salvatore M. (2005). The many ways to myocardial perfusion imaging. Q J Nucl Med Mol Imaging.
2 Flotats A., Carrio I. (2003). Non-invasive in vivo imaging of myocardial apoptosis and necrosis. Eur J Nucl Med Mol Imaging.
3 Taki J. Matsunari I. Metabolic imaging using SPECT Eur J Nucl Med Mol Imaging 2007 34Suppl 1S34 48 17479263
4 Lin Q., Luo H., Mokler F., Beets A.L., Ambrose K.R., McPherson D.W., Kropp J., Knapp F.F. (1997). Effects of configuration on the myocardial uptake of radioiodinated 3(R)-BMIPP and 3(S)-BMIPP in rats. J Nucl Med.
5 Pastore C.J. Babich J.W. Udelson J.E. Future directions of myocardial fatty acid imaging J Nucl Cardiol 2007 14Suppl3 S153 63 17556184
6 Magro C.M., Abbas A.E., Ross P. (2006). The application of photodynamic therapy in the treatment of metastatic endobronchial disease. Lasers Surg Med.
7 Lee S.S., Goo H.W., Park S.B., Lim C.H., Gong G., Seo J.B., Lim T.H. (2003). MR imaging of reperfused myocardial infarction: comparison of necrosis-specific and intravascular contrast agents in a cat model. Radiology.
8 Choi S.I., Choi S.H., Kim S.T., Lim K.H., Lim C.H., Gong G.Y., Kim H.Y., Weinmann H.J., Lim T.H. (2000). Irreversibly damaged myocardium at MR imaging with a necrotic tissue-specific contrast agent in a cat model. Radiology.
9 Bormans G., Huyghe D., Christiaen A., Verbeke K., de Groot T., Vanbilloen H., de Witte P., Verbruggen A. (2004). Preparation, analysis and biodistribution in mice of iodine-123 laballed derivatives of hypericin. J Label Comp Radiopharm.
10 Fonge H., Van de Putte M., Huyghe D., Bormans G., Ni Y., de Witte P., Verbruggen A. (2007). Evaluation of tumor affinity of mono-[(123)I]iodohypericin and mono-[(123)I]iodoprotohypericin in a mouse model with a RIF-1 tumor. Contrast Media Mol Imaging.
11 Fonge H., Vunckx K., Wang H., Feng Y., Mortelmans L., Nuyts J., Bormans G., Verbruggen A., Ni Y. (2008). Non-invasive detection and quantification of acute myocardial infarction in rabbits using mono-[123I]iodohypericin {micro}SPECT. Eur Heart J.
12 Ni Y., Huyghe D., Verbeke K., de Witte P.A., Nuyts J., Mortelmans L., Chen F., Marchal G., Verbruggen A.M., Bormans G.M. (2006). First preclinical evaluation of mono-[123I]iodohypericin as a necrosis-avid tracer agent. Eur J Nucl Med Mol Imaging.
13 Fonge H., Jin L., Wang H., Ni Y., Bormans G., Verbruggen A. (2007). Synthesis and preliminary evaluation of mono-[123I]iodohypericin monocarboxylic acid as a necrosis avid imaging agent. Bioorg Med Chem Lett.
14 Marie P.Y., Menu P., Angioi M., Mertes P.M., Ayalew A., Hassan N., Olivier P., Fagret D., Karcher G., Danchin N., Pasqualini R., Bertrand A. (1999). The kinetics of beta-methyl-substituted labelled fatty acids in ischaemic myocardium: an analysis in man and with a blood-perfused isolated heart model. Eur J Nucl Med.